# ^99m^Tc(CO)_3_-Bipyridine-cyclo-(Arg-Gly-Asp-D-Tyr-Lys)

Chemical name: | ^99m^Tc-Bipyridine-cyclo-(Arg-Gly-Asp-D-Tyr-Lys)
Abbreviated name: | ^99m^Tc(CO)_3_-BPy-c(RGDyK), ^99m^Tc(CO)_3_-BPy-RGD
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+BPy-RGD)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell-cell and cell-matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents and the agonists as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most of the cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (IC_50_, 7-40 nM) but not to α_v_β_5_ (IC_50_, 600-4,000 nM) or α_IIb_β_3_ (IC_50_, 700-5,000 nM) integrins. Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). The ready availability and low cost of ^99m^Tc led to the development of ^99m^Tc-RGD peptides for targeting α_v_β_3_ integrins in tumor angiogenesis. ^99m^Tc(CO)_3_-Bipyridine-cyclo-(Arg-Gly-Asp-D-Tyr-Lys) (^99m^Tc(CO)_3_-BPy-c(RGDyK)) has been prepared as a single-photon emission computed tomography (SPECT) tracer for imaging α_v_β_3_ integrins in tumor (13).

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+BPy-RGD+and+synthesis)]

5-Carboxylate-2,2’-bipyridine (BPy) was conjugated to the ε amino group of Lys of c(RGDyK) to form BPy-c(RGDyK). ^99m^Tc(CO)_3_–BPy–c(RGDyK) was prepared by exchange reaction between [^99m^Tc(H_2_O)_3_(CO)_3_]^+^ and BPy–c(RGDyK) at 70°C for 20 min and purified by high-performance liquid chromatography (13). The radiochemical purity of >98% was obtained, and the radiochemical yield was ~70%. The specific activity was 20 GBq/μmol (0.54 Ci/μmol) at the end of purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+BPy-RGD+and+in+vitro)]

A receptor-binding assay with ^125^I-echistatin was established using MDA-MB-435 breast cancer cell line, which contains α_v_β_3_ integrins (14). Zhang et al. (13) reported that c(RGDyK) and BPy-c(RGDyK) had IC_50_ values of 59.07 ± 11.03 and 92.51 ± 22.69 nM, respectively. Haubner et al. (11) showed that c(RGDyK(SAA)) had IC_50_ values of 20, 4,000, and 3,000 nM for α_v_β_3_, α_v_β_5_, and α_IIb_β_3_, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+BPy-RGD+and+rodentia)]

Zhang et al. (13) performed biodistribution studies of ^99m^Tc(CO)_3_–BPy– c(RGDyK) in nude mice, using an orthotopic MDA-MB-435 breast tumor xenograft model. Data were obtained at 1.5, 4, and 8 h after injection. The initial tracer accumulation in the α_v_β_3_-integrin-expressing tumor was 1.45 ± 0.25% ID/g at 1.5 h and decreased to 0.11 ± 0.01% ID/g at 8 h. Tumor uptake of radioactivity was blocked (53% inhibition) by co-injection of unlabeled c(RGDyK) (10 mg/kg) from 0.71% ID/g to 0.33% ID/g at 4 h after injection. At 1.5 h, the highest radioactive concentration was found in the liver (13.57% ID/g), followed by the kidney, lung, spleen and intestine. The tumor uptakes at 1.5 h after injection were 0.36 ± 0.04% ID/g for ^99m^Tc(CO)_3_–BPy–CO_2_H and 0.29 ± 0.02% ID/g for ^99m^Tc(CO)_3_(H_2_O)_3_^+^, which were significantly lower than that of ^99m^Tc(CO)_3_–BPy–RGD at the same time point (p<0.001). Both ^99m^Tc(CO)_3_–BPy–CO_2_H and ^99m^Tc(CO)_3_(H_2_O)_3_^+^ had high and persistent radioactivity accumulation in the liver and kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+BPy-RGD+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+BPy-RGD+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+BPy-RGD+and+human)]

No publication is currently available.

## NIH Support

P50 CA114747, R21 CA102123, R21 EB001785, R24 CA93862

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Zhang X., Chen X. (2007). Preparation and characterization of 99mTc(CO)3-BPy-RGD complex as alphav beta3 integrin receptor-targeted imaging agent. Appl Radiat Isot.
14 Zitzmann S., Ehemann V., Schwab M. (2002). Arginine-glycine-aspartic acid (RGD)-peptide binds to both tumor and tumor-endothelial cells in vivo. Cancer Res.